# Gd-DTPA-Cystine diethyl ester copolymers

Chemical name: | Gd-DTPA-Cystine diethyl ester copolymers
Abbreviated name: | GDCEP
Synonym:
Agent Category: | Compound
Target: | Non-targeted
Target Category: | Blood pool retention
Method of detection: | Magnetic resonance imaging, MRI
Source of signal\contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%5BAll%20Fields%5D)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises about 80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclei (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents, which contain chemical moiety with unpaired electrons affecting the T1 and T2 relaxation times of the surrounding nuclei, predominantly the protons of water (1). MRI contrast agents work by shortening both T1 and T2 relaxation times of surrounding water protons to produce the signal-enhancing effect (2, 3), highlight vasculature, and delineate normal or nonmalignant tissues (4).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-Diethylenetriaminepentaacetate (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their application as imaging agents in the vasculature and cancer. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (4, 7, 8); however, these Gd complexes cannot proceed into further clinical development because of their slow excretion and high tissue accumulation of toxic Gd ions.

New, biodegradable, macromolecular Gd complexes, which can be readily degraded to smaller complexes for faster excretion through renal filtration, are being developed as MRI contrast agents (9). Gd-DTPA cystine copolymers (GDCP) and Gd-DTPA cystine diethyl ester copolymers (GDCEP) are biodegradable polydisulfide Gd(III) complexes that are readily degraded by a disulfide-thio exchange reaction (10-12). GDCP and GDCEP are being developed as contrast-enhanced MRI agents for use in blood pool and cancer imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20synthesis)]

Zong et al. (12) reported that the synthesis of GDCP and GDCEP consisted of two major steps. DTPA dianhydride was first copolymerized with cystine or cystine diethyl ester, and then complexed with GdCl_3_ via DTPA to form GDCP and GDCEP, respectively. The yields of GDCP and GDCEP were 15% and 11%, respectively. The average molecular weight (M_w_) of GDCP was 15.1 kDa; the average M_w_ of GDCEP was 10.2 kDa. The measured Gd contents in GDCP and GDCEP were 19.5% and 18.2%, respectively. The longitudinal T1 relaxivity (r_1_) at 3T was 5.43 mM^-1^s^-1^ for GDCP and 5.86 mM^-1^s^-1^ for GDCEP.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20in%20vitro)]

Both GDCP and GDCEP rapidly degraded in vitro during incubation with a high concentration of cysteine (150 μM) at 37°C (12). Most of the copolymers degraded into smaller oligomers and complexes at 6 h, and eventually degraded to the smallest repeat unit of the copolymers, Gd-[DTPA-(cysteine)_2_] and Gd-DTPA-[(cysteine ethyl ester)_2_], as determined by mass spectroscopy. The r_1_ of the degradation products of GDCP and GDCEP were 5.39 and 5.70 mM^-1^s^-1^, respectively. Compared with GDCP, GDCEP showed more rapid degradation into smaller units in rat blood plasma as in the presence of cysteine (11). About 10% of GDCP degraded into smaller GD complexes in 6-h incubation, while >60% of GDCEP degraded in 1-h incubation. Little free Gd was detected.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20rodentia)]

In mice and rats, GDCP and GDCEP rapidly distributed into the blood and vascular compartments, and both showed a marked affinity for renal excretion (10-12). The biodistribution study showed that both were found mainly in the liver, kidneys, spleen, and heart. GDCP and GDCEP degradation was confirmed in the urinary samples of rats. Pharmacokinetic studies of GDCEP, GDCP, and the nondegradable macromolecular copolymer Gd-DTPA-1,6-hexanediamine copolymer (GDHC) (0.1 mmol/kg) were conducted in rats by Feng et al. (10), who found that the blood kinetics [distribution half-life (t_½_), α; elimination t_½_, β] were 1.60 ± 0.73 min (α) and 29.3 ± 15.9 min (β), 3.15 ± 1.26 min (α) and 33.1 ± 19.3 min (β), and 5.92 ± 2.02 min (α) and 222.6 ± 63.9 min (β), for GDCP, GDCEP, and GDHC, respectively. The rank order of blood retention was GDHC>>GDCP>GDCEP, which corresponded to the degrees of nondegradation of the copolymers. The α phase of GDCP was significantly longer than that of GDCEP (P < 0.05). The accumulation of GDHC in the muscle, liver, kidney, and spleen was higher than that of GDCP and GDCEP, and GDCP exhibited significantly higher accumulation in these organs than did GDCEP. GDHC showed stronger and more prolonged contrast enhancement than GDCP and GDCEP in the heart and blood vessels in MRI, and GDCP showed longer enhancement duration than GDCEP. On the other hand, GDCP and GDCEP exhibited more significant enhancement in the kidneys than GDHC.

Zong et al. (12) studied MRI using GDCP and GDCEP (0.1 mmol/kg) in nude mice bearing MDA-BM-231 human breast carcinoma xenografts. Gd-DTPA-BMA (bis(methyl)amide), a low molecular weight Gd complex, was used as a control. GDCP and GDCEP resulted in strong contrast enhancement in the blood pool at 5 min after injection. Some blood vessels connected to tumor tissue were clearly visible with both agents. Significant contrast enhancement in the tumor tissues (predominantly in the periphery) was also observed. The tumor contrast enhancement for GDCP rapidly declined after 5 min, and only minimal contrast enhancement was observed at 15 min after injection. The contrast enhancement with GDCEP decreased more gradually in the blood pool, such that significant contrast enhancement was still present at 60 min after injection. No significant contrast enhancement was observed for Gd-DTPA-BMA at 5 min after injection or thereafter.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GDCEP%20and%20human)]

No publication is currently available.

## NIH Support

R33 CA095873, R01 EB00489

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Brasch R.C. (1991). Rationale and applications for macromolecular Gd-based contrast agents. Magn Reson Med.
3 Runge V.M. (1992). Magnetic resonance imaging contrast agents. Curr Opin Radiol.
4 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
8 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
9 Mach R.H., Huang Y., Freeman R.A., Wu L., Vangveravong S., Luedtke R.R. (2004). Conformationally-flexible benzamide analogues as dopamine D3 and sigma 2 receptor ligands. Bioorg Med Chem Lett.
10 Feng Y., Zong Y., Ke T., Jeong E.K., Parker D.L., Lu Z.R. (2006). and Pharmacokinetics, biodistribution and contrast enhanced MR blood pool imaging of Gd-DTPA cystine copolymers and Gd-DTPA cystine diethyl ester copolymers in a rat model. Pharm Res.
11 Zong Y., Guo J., Ke T., Mohs A.M., Parker D.L., Lu Z.R. (2006). Effect of size and charge on pharmacokinetics and in vivo MRI contrast enhancement of biodegradable polydisulfide Gd(III) complexes. J Control Release.
12 Zong Y., Wang X., Goodrich K.C., Mohs A.M., Parker D.L., Lu Z.R. (2005). Contrast-enhanced MRI with new biodegradable macromolecular Gd(III) complexes in tumor-bearing mice. Magn Reson Med.